# Hyperpolarized [1,4-^13^C_2_]fumarate as an imaging agent of tumor cell death in vivo

Chemical name: | Hyperpolarized [1,4-^13^C_2_]fumarate
Abbreviated name: | [1,4-^13^C_2_]Fumarate
Synonym:
Agent Category: | Compounds
Target: | Fumarase (or fumarate hydratase)
Target Category: | Enzymes
Method of detection: | Magnetic resonance imaging (MRI)/magnetic resonance spectroscopy (MRS)
Source of signal / contrast: | Hyperpolarized ^13^C
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Magnetic+resonance+spectroscopy)]

Magnetic resonance spectroscopy (MRS) is a technique that allows us to non-invasively detect multiple small metabolites within cells or extracellular spaces in vivo (1-3). The clinical use of MRS as an adjunct to magnetic resonance imaging (MRI), particularly in cancer detection and treatment response evaluation, has expanded dramatically over the past several years. Although MRS is theoretically applicable to any nucleus possessing spin, the most important and more frequently investigated applications are in proton (^1^H) and carbon-13 (^13^C) (4-6). ^13^C MRS is superior to ^1^H MRS in many respects (3, 6-8). ^13^C MRS can provide specific information about the identity and structure of biologically important compounds. The chemical shift range for carbon (~250 ppm) is much larger than that for proton (~15 ppm), allowing for improved resolution of metabolites. In addition, the T_1_ relaxation time of ^13^C in small molecules is much longer than that of ^1^H (0.1–2.0 s in a magnetic field of 0.1–3.0 T), allowing the generation of hyperpolarized ^13^C-labeled tracers outside the subject and the MRI scanner. Some of these tracers are endogenous and therefore have lower toxicity than drugs and exogenous contrast media (6). However, ^13^C MRS is limited by the low natural abundance of ^13^C (1.1%) and its low magnetogyric ratio (γ of ^13^C is one quarter that of ^1^H) (2, 3).

Several techniques have been used to overcome the ^13^C MRS limitation through enhancing the polarization of nuclear spins. One technique is proton decoupling, which eliminates the coupling of ^1^H with ^13^C by irradiating the entire ^1^H resonance absorption range and consequently collapsing ^13^C resonances to singlets (4, 5). The signal/noise ratio of ^13^C resonances has been shown to be significantly increased with proton decoupling. Another technique is known as dynamic nuclear polarization (DNP), which introduces one or more ^13^C molecules into a metabolic substrate (2, 3, 8). DNP transfers high electron spin polarization to nuclear spins via microwave irradiation. Nearly 100% nuclear polarization for ^1^H and 50% for ^13^C can be achieved in various organic molecules when DNP is performed in a strong magnetic field and at cryogenic temperatures. Replacing the ^12^C (98.9% natural abundance) isotope with the ^13^C isotope at a specific carbon or carbons in a metabolic substrate does not affect the substrate's biochemistry. With ^13^C MRS, the body tissues are virtually invisible, and only regions where the hyperpolarized ^13^C-labeled substance is present will appear in the generated images. Thus, ^13^C-labeled substrates can provide >10,000-fold enhancement of the ^13^C MRS signals from the substrate and its subsequent metabolic products, allowing the assessment of changes in metabolic fluxes in vivo through glycolysis, citric acid cycle, and fatty acid synthesis (1, 9-13). Vascular and perfusion imaging can also be performed without background signal from surrounding tissues (3, 14).

Gallagher et al. generated a hyperpolarized small molecule, [1,4-^13^C_2_]fumarate, as an imaging agent of ^13^C MRS for evaluation of early tumor response to treatment and other pathological states in which cell death plays a role, such as toxic insults or ischemia (1). Fumarate, a tricarboxylic acid cycle intermediate, is hydrated to produce malate in a reaction catalyzed by fumarase (or fumarate hydratase). The transport of fumarate across the plasma membrane is mediated by the sodium-dependent dicarboxylate acid transporter, which also transports succinate. Fumarate transport across the mitochondrial membrane occurs in exchange for malate, inorganic phosphate, or aspartate. The reaction enzyme fumarase exists as both cytosolic and mitochondrial isoforms, and the relative activity of the two isoforms varies markedly between tissues and between species. The investigators showed that [1,4-^13^C_2_]malate production from [1,4-^13^C_2_]fumarate is increased in treated lymphoma cells and tumors, and that this increase is caused by tumor cell necrosis. The formation of hyperpolarized [1,4-^13^C_2_]malate from [1,4-^13^C_2_]fumarate appears to be a sensitive marker of tumor cell death in vivo and could be used to detect the early response of tumors to treatment (1).

### Related Resource Links:

- Chapters of ^13^C MRS in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=13C%2C+MRI+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Fumarase in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=136850)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Magnetic+resonance+spectroscopy+and+fumarate+and+malate+cell+necrosis)]

Gallagher et al. detailed the generation of hyperpolarized [1,4-^13^C_2_]fumarate (1). Briefly, commercially available [1,4-^13^C_2_]fumaric acid was dissolved in dimethyl sulfoxide containing trityl radical and gadolinium chelate. The solution was sonicated, centrifuged, and then hyperpolarized. The hyperpolarized [1,4-^13^C_2_]fumarate was dissolved in buffer containing 40 mmol phosphate, 50 mmol sodium chloride, and 40 mmol sodium hydroxide (pH 7.4) at 10 bar and 180°C. The resulting solution contained 20 mmol [1,4-^13^C_2_]fumarate, and it was then cooled to ~37°C before injection. The polarization of [1,4-^13^C_2_]fumarate was between 26% and 35%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Magnetic+resonance+spectroscopy+and+fumarate+and+malate+cell+necrosis)]

Gallagher et al. first analyzed the conversion of [1,4-^13^C_2_]fumarate to [1,4-^13^C_2_]malate in the cell cultures of EL4 murine lymphoma cells with or without etoposide pretreatment (1). Etoposide pretreatment results in an increase in the combined apoptosis and necrosis of tumor cells. EL4 cells (5 × 10^7^) resuspended in 2 ml medium were then placed in a 10-mm nuclear magnetic resonance tube. The hyperpolarized [1,4-^13^C_2_]fumarate solution alone or in combination with sodium succinate was injected into the cell suspension via a fine bore tube. Succinate is transported into the cells on the same transporter as fumarate and thus competes with fumarate. ^13^C spectra were acquired at 9.4 T with proton-decoupling and low flip-angle radiofrequency pulses.

In the ^13^C spectra, [1,4-^13^C_2_]fumarate produced a single peak, whereas [1,4-^13^C_2_]malate gave two resonances because the carbons were not equivalent. The rate constants k_F_ and k_M_ were calculated; k_F_ was the apparent rate constant for the conversion of fumarate to malate, and k_M_ was the apparent rate constant for the reverse reaction. It is worth noting that k_F_ and k_M_ not only described flux in the fumarase-catalyzed reaction but also substrate transport across the plasma and mitochondrial membranes in this study. The decay of hyperpolarization in [1,4-^13^C_2_]fumarate and [1,4-^13^C_2_]malate was described by the time constants T_F_ and T_M_, respectively. T_F_ was calculated to be 24.1 ± 2.1 s (n = 18), and T_M_ was calculated to be 18.4 ± 7.0 s (n = 12) without significant difference (P < 0.01) between them. After injection of [1,4-^13^C_2_]fumarate into the cell suspensions, signal from hyperpolarized [1,4-^13^C_2_]malate was observed; however, the malate signal in untreated cells was only slightly discernable. At 16 h after treatment of the cells with etoposide, there was a large increase in the rate of malate production. The k_F_ was 19 times higher in the etoposide-treated cells (0.056 ± 0.053 × 10^-10^s^-1^ cell^-1^; n = 3) than in the untreated cells (0.003 ± 0.002 × 10^-10^ s^-1^cell^-1^; n = 3 (P < 0.01)). When the cells were lysed with freeze-thawing, there was a further increase in the rate of malate production (0.177 ± 0.017 × 10^-10^ s^-1^cell^-1^; n = 3), 62 times higher than in the untreated group (P < 0.01). Coadministration of succinate had no significant effect on the rate of labeled malate production. However, it was difficult to determine whether succinate had an effect in untreated cells because of the low level of malate production. Cell necrosis was also measured with trypan blue at the end of these flux determinations. There was a good correlation between the rate of malate production and the level of necrosis (R^2^ = 0.89).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Magnetic+resonance+spectroscopy+and+fumarate+and+malate+cell+necrosis)]

Gallagher et al. performed imaging studies in female C57BL/6 mice bearing subcutaneous EL4 tumors (1). Hyperpolarized [1,4-^13^C_2_]fumarate was injected via a tail vein catheter over a period of 6 s. ^13^C spectra were acquired at 2.35 T. After injection of the [1,4-^13^C_2_]fumarate, the signals from [1,4-^13^C_2_]fumarate, [1-^13^C]malate, and [4-^13^C]malate were seen at 175.4, ~181.8, and ~180.6 ppm, respectively. Production of malate was heterogeneous within the tumor. Some areas of the tumor showed a low fumarate signal, despite the presence of significant labeled malate production. This low fumarate signal might be caused by variations in tissue perfusion and rapid fumarate consumption because highly necrotic areas are likely to have poor perfusion and high extracellular fumarase activity, which may rapidly convert the small amount of fumarate to malate. The signal from [1,4-^13^C_2_]malate was observed in both untreated (n = 5) and treated (n = 5) EL4 tumors at 24 ± 2 h after etoposide administration. When normalized to the maximum fumarate signal, the maximum malate signal was 59% higher in the treated (0.23 ± 0.04) than in the untreated tumors (0.15 ± 0.04; P < 0.01). The fumarate signal peaked at approximately the same time in treated and untreated tumors, but there was a more rapid signal decline in the treated group. The k_F_ was 2.5-fold higher in the treated tumors (0.018 ± 0.004 s^-1^) than in the untreated tumors (0.007 ± 0.002 s^-1^) (n = 5 mice; P < 0.001). There was a similar increase in the reverse rate constant (k_M_) in the treated group (0.018 ± 0.005 s^-1^) compared with the untreated groups (0.007 ± 0.006 s^-1^; P < 0.05). The similarity of the relative changes in the forward and reverse rate constants was consistent with an increase in the concentration of fumarase available to its substrates. There was no difference in the calculated rate of flow of the hyperpolarized fumarate into the tumor between the treated (0.27 ± 0.14 s^-1^) and the untreated groups (0.19 ± 0.05 s^-1^; P = 0.23). There was also no significant difference in T_F_ (and hence T_M_) between the treated (36.7 ± 3.3 s) and the untreated (40.1 ± 2.7 s) animals (n = 5; P = 0.11). The difference between these values and those obtained in vitro could be explained by the different field strengths used for these experiments (2.35 versus 9.4 T).

^13^C chemical shift images acquired at ~30 s showed that the fumarate could be observed throughout the animals, but that the hyperpolarized malate signal was found predominately within the tumors. The maximum malate signal was seen at 33 ± 4 s in the untreated animals and at 27 ± 2 s in the treated animals (P < 0.01).

The separate experiments at 9.4 T demonstrated that only ~2% of the total hyperpolarized ^13^C signal was seen as malate outside the tumor. The average malate/fumarate ratios in the liver were 0.020 ± 0.019 (n = 3 tumor-bearing animals before treatment), 0.020 ± 0.017 (n = 3 tumor-bearing animals 24 h after treatment), 0.022 ± 0.016 (n = 3 control animals before treatment), and 0.017 ± 0.007 (n = 2 control animals 24 h after treatment). There was no significant difference between these groups (P > 0.66), which confirmed that the majority of the malate signal came from the tumor rather than being washed in from another organ, such as the liver.

Measurement of the fumarase activities in tissue extracts showed a significantly lower fumarase activity in the treated tumors (277 ± 18 U/g protein, n = 6) than in the untreated tumors (319 ± 30 U/g protein, n = 5 (P = 0.02)). The fumarase activity in muscle from the control animals was 312 ± 35 U/g protein (n = 4). There was also significantly lower malate dehydrogenase (MDH) activity in treated tumors (227 ± 32 U/g protein, n = 6) than in untreated tumors (274 ± 20 U/g protein, n = 5 (P = 0.02)), and both were significantly lower than muscle MDH activity (340 ± 38 U/g protein, n = 4 (P < 0.01) in both cases).

The increase in labeled malate production in treated tumors cannot be explained by changes in fumarase activity, because a decrease in enzyme activity was observed in the extracts of treated tumors. However, the increase in labeled malate production can be explained by increased access of fumarate to the enzyme because of increased plasma membrane permeability of the necrotic tumor cells. Consistent with this explanation, the presence of succinate had no effect on the rate of label flux between fumarate and malate. Increased malate production could also be caused by mitochondrial membrane rupture, which occurs before plasma membrane damage after the onset of necrosis and releases the enzyme into the cytosol (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Gallagher F.A., Kettunen M.I., Hu D.E., Jensen P.R., Zandt R.I., Karlsson M., Gisselsson A., Nelson S.K., Witney T.H., Bohndiek S.E., Hansson G., Peitersen T., Lerche M.H., Brindle K.M. (2009). Production of hyperpolarized [1,4-13C2]malate from [1,4-13C2]fumarate is a marker of cell necrosis and treatment response in tumors. Proc Natl Acad Sci U S A.
2 Kurhanewicz J., Bok R., Nelson S.J., Vigneron D.B. (2008). Current and potential applications of clinical 13C MR spectroscopy. J Nucl Med.
3 Mansson S., Johansson E., Magnusson P., Chai C.M., Hansson G., Petersson J.S., Stahlberg F., Golman K. (2006). 13C imaging-a new diagnostic platform. Eur Radiol.
4 Chen A.P., Tropp J., Hurd R.E., Van Criekinge M., Carvajal L.G., Xu D., Kurhanewicz J., Vigneron D.B. (2009). In vivo hyperpolarized 13C MR spectroscopic imaging with 1H decoupling. J Magn Reson.
5 Ardenkjaer-Larsen J.H., Fridlund B., Gram A., Hansson G., Hansson L., Lerche M.H., Servin R., Thaning M., Golman K. (2003). Increase in signal-to-noise ratio of > 10,000 times in liquid-state NMR. Proc Natl Acad Sci U S A.
6 Golman K., Ardenkjaer-Larsen J.H., Petersson J.S., Mansson S., Leunbach I. (2003). Molecular imaging with endogenous substances. Proc Natl Acad Sci U S A.
7 Larson P.E., Kerr A.B., Chen A.P., Lustig M.S., Zierhut M.L., Hu S., Cunningham C.H., Pauly J.M., Kurhanewicz J., Vigneron D.B. (2008). Multiband excitation pulses for hyperpolarized 13C dynamic chemical-shift imaging. J Magn Reson.
8 Golman K., Olsson L.E., Axelsson O., Mansson S., Karlsson M., Petersson J.S. (2003). Molecular imaging using hyperpolarized 13C. Br J Radiol.
9 Albers M.J., Bok R., Chen A.P., Cunningham C.H., Zierhut M.L., Zhang V.Y., Kohler S.J., Tropp J., Hurd R.E., Yen Y.F., Nelson S.J., Vigneron D.B., Kurhanewicz J. (2008). Hyperpolarized 13C lactate, pyruvate, and alanine: noninvasive biomarkers for prostate cancer detection and grading. Cancer Res.
10 Chen A.P., Kurhanewicz J., Bok R., Xu D., Joun D., Zhang V., Nelson S.J., Hurd R.E., Vigneron D.B. (2008). Feasibility of using hyperpolarized [1-13C]lactate as a substrate for in vivo metabolic 13C MRSI studies. Magn Reson Imaging.
11 Gallagher F.A., Kettunen M.I., Day S.E., Hu D.E., Ardenkjaer-Larsen J.H., Zandt R., Jensen P.R., Karlsson M., Golman K., Lerche M.H., Brindle K.M. (2008). Magnetic resonance imaging of pH in vivo using hyperpolarized 13C-labelled bicarbonate. Nature.
12 Karlsson, M., P.R. Jensen, R.I. Zandt, A. Gisselsson, G. Hansson, J.O. Duus, S. Meier, and M.H. Lerche, Imaging of branched chain amino acid metabolism in tumors with hyperpolarized (13)C ketoisocaproate. Int J Cancer, 2009
13 Jensen P.R., Karlsson M., Meier S., Duus J.O., Lerche M.H. (2009). Hyperpolarized amino acids for in vivo assays of transaminase activity. Chemistry.
14 Olsson L.E., Chai C.M., Axelsson O., Karlsson M., Golman K., Petersson J.S. (2006). MR coronary angiography in pigs with intraarterial injections of a hyperpolarized 13C substance. Magn Reson Med.